# ^86^Y-CHX-A''-Diethylenetriamine pentaacetic acid-cetuximab

Chemical name: | ^86^Y-CHX-A''-Diethylenetriamine pentaacetic acid-cetuximab
Abbreviated name: | ^86^Y-CHX-A''-DTPA-cetuximab
Synonym: | ^86^Y-CHX-A''-DTPA-erbitux
Agent category: | Chimeric monoclonal antibody
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^86^Y
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4503491), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001963.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1950) for more information about EGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20Cetuximab)]

Epidermal growth factor (EGF) is a 53-amino acid cytokine (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab, a humanized immunoglobulin G_1_ (IgG_1_) monoclonal antibody against the extracellular domain of recombinant HER2 (11), was labeled as ^111^In-trastuzumab (12-14). C225, an anti-EGFR (HER1), mouse-human chimeric, monoclonal IgG_1_ antibody, also known as erbitux and cetuximab, was labeled as ^99m^Tc-EC-C225 (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=EC-C225-99mtc) (15, 16) for imaging EGFR expression on solid tumors using single-photon emission computed tomography (SPECT). For evaluation as a positron emission tomography (PET) imaging agent for EGFR, ^86^Y has been attached to cetuximab via CHX-A''-diethylenetriamine pentaacetic acid (CHX-A''-DTPA) to form ^86^Y-CHX-A''-DTPA-cetuximab (17).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550)
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20Cetuximab%20and%20synthesis)]

Bifunctional CHX-A''-DTPA was used to conjugate cetuximab to form CHX-A''-DTPA-cetuximab (~150 kD), which was purified with column chromatography (17). DTPA per antibody was determined to be 2.3. Next, ^86^Y solution (140–170 MBq (3.8–4.6 mCi)) was added to CHX-A''-DTPA-cetuximab (0.33 nmol) in ammonium acetate buffer (pH 5–6). The reaction mixture was incubated for 30 min at room temperature, and ^86^Y-CHX-A''-DTPA-cetuximab was purified with column chromatography. The yield of ^86^Y-CHX-A''-DTPA-cetuximab was 55%–75% with a specific activity of ~300 MBq/nmol (8.1 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20Cetuximab%20and%20in%20vitro)]

Nayak et al. (17) performed cell-binding assays with ^86^Y-CHX-A''-DTPA-cetuximab using the EGFR-expressing human glioblastoma U87MG cell line. Binding of ^86^Y-CHX-A''-DTPA-cetuximab under excess antigen conditions indicated that the immunoreactivity was 65%–75%, suggesting that the majority of the accessible lysine residues were some distance from the EGFR-binding region of cetuximab. ^86^Y-CHX-A''-DTPA-cetuximab was stable for up to 24 h in buffer at 4°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20Cetuximab%20and%20rodentia)]

Nayak et al. (17) performed ex vivo biodistribution studies of 0.5 MBq (0.014 mCi) ^86^Y-CHX-A''-DTPA-cetuximab in nude mice (n = 5) bearing human colorectal carcinoma LS-174T tumors at 1–4 d after injection. Accumulation into LS-174T tumors was high, with 21.2 ± 1.0% injected dose/gram (ID/g) at 1 d and 27.4 ± 3.6% ID/g at 4 d after injection. On the other hand, normal tissues exhibited gradual declines in radioactivity from 1 d (<10% ID/g) to 4 d (<5% ID/g) after injection. Radioactivity declined by 70% in the blood and by 60% in the liver from 1 d to 4 d after injection. The tumor/blood ratio increased from 1.5 at 1 d to 6.8 at 4 d after injection. Co-injection of 1.3 nmol cetuximab inhibited the tumor accumulation by ~78% at 3 d after injection. By contrast, little inhibition was observed in the non-tumor tissues.

Nayak et al. (17) studied the whole-body distribution of 4 MBq (0.11 mCi) ^86^Y-CHX-A''-DTPA-cetuximab with microPET imaging in six xenograft (EGFR-positive) tumor models in mice with static scans at various time points (1–3 d). The tumor uptake reached a plateau at 2 d after injection. The accumulation of ^86^Y-CHX-A''-DTPA-cetuximab was clearly visible in all tumors at 1–3 d after injection. The mean tumor residence times were similar in all six tumors (2.1–2.5 d). Co-injection of 1.3 nmol cetuximab inhibited accumulation of radioactivity in the LS-174T tumors by 76% at 3 d after injection. There was a good correlation (r^2^ = 0.9) between the tracer accumulation measured with microPET and that measured with ex vivo biodistribution studies.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20Cetuximab%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20Cetuximab%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20Cetuximab%20and%20human)]

No publication is currently available.

## NIH Support

Intramural research program

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
16 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
17 Nayak T.K., Regino C.A., Wong K.J., Milenic D.E., Garmestani K., Baidoo K.E., Szajek L.P., Brechbiel M.W. (2010). PET imaging of HER1-expressing xenografts in mice with 86Y-CHX-A''-DTPA-cetuximab. Eur J Nucl Med Mol Imaging.